# [S-methyl-^11^C]N,N-Dimethyl-4-(6-(methylthio)imidazo[1,2-a]pyridine-2-yl)aniline

Chemical name: | [S-methyl-^11^C]N,N-Dimethyl-4-(6-(methylthio)imidazo[1,2-a]pyridine-2-yl)aniline
Abbreviated name: | [^11^C]MeS-IMPY
Synonym:
Agent Category: | Compound
Target: | Aggregates of ß-amyloid (Aß) peptides
Target Category: | Acceptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MeS-IMPY)]

Alzheimer’s disease (AD) is a major neurodegenerative disease associated with an irreversible decline of mental functions and with cognitive impairment (1). It is characterized pathologically by neuronal loss with the presence in the brain of senile plaques of β-amyloid (Aβ) peptides and intracellular neurofibrillary tangles of filaments that contain the hyperphosphorylated protein tau (2, 3). Accelerated deposition of Aβ deposits seems to be a key risk factor associated with AD.

Early diagnosis of AD is important for treatment consideration and disease management (4). Several radioligands [PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=amyloid+plaque+and+radioisotopes)] for positron emission tomography (PET) have been developed (5-7) and tested in humans as in vivo diagnostic tools for imaging and measuring the formation of Aβ deposits (7). The first agent successfully used in human studies was [^18^F]FDDNP (8), a malonitrile derivative found to bind to both neurofibrillary tangles and Aβ plaques. The second successful agent was [^11^C]PIB (9), also known as Pittsburgh Compound B or [^11^C]6-OH-BTA-1, which showed marked retention in areas of the cortex known to contain substantial amounts of Aβ deposits. The third PET radioligand successfully tested in humans was [^11^C]4-N-methylamino-4’-hydroxystilbene ([^11^C]SB-13), a stilbene derivative that exhibits good binding affinities for Aβ aggregates in vitro, moderate lipophilicity, high initial brain uptake in the normal rat cortex, and a rapid washout (10).

[^125^I]6-Iodo-2-(4’-dimethylamino)-phenyl-imidazo[1,2-a]pyridine ([^125^I]IMPY) displays a high specific binding for Aβ plaques and favorable brain uptake kinetics in rodents for single-photon emission computed tomography (SPECT). [S-methyl-^11^C]N,N-Dimethyl-4-(6-(methylthio)imidazo[1,2-a]pyridine-2-yl)aniline ([^11^C]MeS-IMPY) has been synthesized as an S-methyl analog of [^125^I]IMPY and is currently being studied as a PET radioligand for Aβ plaques (11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MeS-IMPY%20and%20synthesis)]

[^11^C]MeS-IMPY was synthesized from its precursor by S-methylation in acetonitrile with the use of ^11^C-methyl iodide (80°C for 5 min) (11). [^11^C]MeS-IMPY was purified by reversed-phase high-performance liquid chromatography with >98% radiochemical purity. The radiochemical yields (decay-corrected) on the basis of [^11^C]CO_2_ were 10–15% , and the specific activities were 37–148 GBq/µmol (1.0–4.0 Ci/µmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MeS-IMPY%20and%20in%20vitro)]

MeS-IMPY was found to have an inhibition constant (K_i_) value of 7.93 nM using human AD brain homogenates (11). MeS-IMPY exhibited a moderate lipophilicity (log D value of 4.1 at pH 7.4). These values are comparable to those of IMPY (K_i_ value of 8.95 nM and log D value of 3.58).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MeS-IMPY%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MeS-IMPY%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MeS-IMPY%20and%20%28primate%20not%20human%29)]

Seneca et al. (11) studied PET imaging in the brains of five young male rhesus monkeys after intravenous injection of 191 ± 75 MBq (5.16 ± 2.03 mCi) [^11^C]MeS-IMPY. Various brain regions exhibited rapid accumulation with rapid decreases thereafter. [^11^C]MeS-IMPY PET images (up to 120 min after injection) showed high standardized uptake values of ~500% and ~600% at 2–3 min in cortical regions and the cerebellum, respectively. The brain uptake of [^11^C]MeS-IMPY was widespread and quite uniform across all cortical regions. Radioactivity rapidly washed out of the brain, with 20% of peak activity remaining at 40 min. Regional brain radioactivity fit well into a one-tissue compartment model. The average volume of distribution in all brain regions was 7.66 ± 2.14 ml/cm^3^ (n = 4). The organs with the highest radiation exposure (μSv/MBq and mrem/mCi) were the gallbladder wall (33.4 and 123.5), urinary bladder (17.0 and 62.9), lungs (12.9 and 47.8), kidneys (11.7 and 43.4), and liver (10.7 and 39.4), with a resulting effective dose of 4.9 μSv/MBq (18.0 mrem/mCi).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MeS-IMPY%20and%20human)]

No publication is currently available.

## NIH Support

Intramural Research Program

## References

1 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
2 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
3 Brandt R., Leschik J. (2004). Functional interactions of tau and their relevance for Alzheimer's disease. Curr Alzheimer Res.
4 de Leon M.J., DeSanti S., Zinkowski R., Mehta P.D., Pratico D., Segal S., Clark C., Kerkman D., DeBernardis J., Li J., Lair L., Reisberg B., Tsui W., Rusinek H. (2004). MRI and CSF studies in the early diagnosis of Alzheimer's disease. J Intern Med.
5 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
6 Bacskai B.J., Hickey G.A., Skoch J., Kajdasz S.T., Wang Y., Huang G.F., Mathis C.A., Klunk W.E., Hyman B.T. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
7 Wu C., Pike V.W., Wang Y. (2005). Amyloid imaging: from benchtop to bedside. Curr Top Dev Biol.
8 Shoghi-Jadid K., Small G.W., Agdeppa E.D., Kepe V., Ercoli L.M., Siddarth P., Read S., Satyamurthy N., Petric A., Huang S.C., Barrio J.R. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
9 Klunk W.E., Engler H., Nordberg A., Wang Y., Blomqvist G., Holt D.P., Bergstrom M., Savitcheva I., Huang G.F., Estrada S., Ausen B., Debnath M.L., Barletta J., Price J.C., Sandell J., Lopresti B.J., Wall A., Koivisto P., Antoni G., Mathis C.A., Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
10 Ono M., Wilson A., Nobrega J., Westaway D., Verhoeff P., Zhuang Z.P., Kung M.P., Kung H.F. (2003). 11C-labeled stilbene derivatives as Abeta-aggregate-specific PET imaging agents for Alzheimer's disease. Nucl Med Biol.
11 Seneca N., Cai L., Liow J.S., Zoghbi S.S., Gladding R.L., Hong J., Pike V.W., Innis R.B. (2007). Brain and whole-body imaging in nonhuman primates with [(11)C]MeS-IMPY, a candidate radioligand for beta-amyloid plaques. Nucl Med Biol.